# ^123/131^I-Anti-cellular adhesion molecule monoclonal antibody 14C5

Chemical name: | ^123/131^I-14C5 monoclonal antibody to cellular adhesion molecule
Abbreviated name: | ^123/131^I-14C5, ^123/131^I-mAb 14C5
Synonym:
Agent category: | Antibody
Target: | Integrin α_v_β_5_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^123^I, ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans surrounding connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM components, which provide a matrix environment for their permeation through the basal lamina and underlying interstitial stroma of the connective tissue. Several ECM adhesion molecules and their protein receptors have been studied extensively for their involvement in tumor invasion and metastasis, including the integrins, lectins, selectins, and cadherins (3).

The monoclonal antibody (mAb) 14C5 recognizes an extracellular membrane antigen expressed on SK-BR-3 human breast tumor cells (4, 5). The 14C5 mAb inhibits the adhesion of tumor cells to ECM and tumor growth. The 14C5 antigen is absent on the cell surface of normal tissues and artery. However, it is present in high amounts on the cell membrane of invasive breast carcinomas and several other malignant tumors (4). Surprisingly, the 14C5 antigen is markedly expressed on the cell surface of fibroblasts surrounding the tumor cells. The 14C5 antigen is determined to have a molecular weight of ~90 kDa and 14C5 binds the vascular integrin α_v_β_5_ (6). ^123/131^I-14C5 is being developed as a non-invasive agent for radioimmunodetection and radioimmunotherapy.

### Related Resource Links:

- Chapters in MICAD (Integrin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Integrin+AND+micad%5Bbook%5D), 14C5 (http://www.ncbi.nlm.nih.gov/books/?term=14C5+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_5_ integrin (http://www.ncbi.nlm.nih.gov/omim/147561))
- Clinical trials (Integrin (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (Integrin (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20synthesis)]

Lahorte et al. (7) performed iodination using IODO beads with 222 MBq (6 mCi) ^123^I and 10 μg 14C5 in phosphate-buffered saline at room temperature for 30 min. Radiochemical yields were 85.0 ± 2.5% after purification with PD-10 column chromatography. Specific activities were ~2.4 ± 0.2 GBq/μmol (65 ± 5 mCi/μmol) with a radiochemical purity of >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20in%20vitro)]

Lahorte et al. (7) reported that ^123^I-14C5 bound to SK-BR-3 cells with a dissociation constant (K_d_) value of 0.85 ± 0.17 nM and to HeLa cells with a K_d_ value of 1.71 ± 0.17 nM with high affinity, and both cell types exhibited a high 14C5 antigen expression (B_max_ = 40.6 ± 5.2 pM and 57.1 ± 9.6 pM, respectively).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20rodentia)]

Lahorte et al. (7) performed ex vivo biodistribution studies of ^123^I-14C5 in normal mice and demonstrated a slow clearance from the blood (9.7 ± 1.4% injected dose per gram (% ID/g) remaining at 48 h after injection) with a biexponential pharmacokinetic behavior. The biexponential blood clearance of ^123^I-14C5 was characterized by a fast distribution phase (half-life α (t_1/2,α_) = 1.43 ± 0.42 h, 62.8% of total circulating radioactivity in the blood) and a slow elimination phase (t_1/2,ß_ = 130.4 ± 100.0 h, 37.2% of total circulating radioactivity in the blood). Blood pool activity was substantially higher than tracer accumulation in any of the other investigated organs at any given time. ^123^I-14C5 did not cross the blood–brain barrier as indicated by the low brain uptake (<1.0% ID/g on average). The highest accumulation of radioactivity occurred in the lungs (20.4 ± 3.7% ID/g), liver (15.1 ± 1.4% ID/g), and kidneys (11.1 ± 1.1% ID/g) within 5 min after injection and to a lesser extent in the spleen (9.2 ± 2.4% ID/g) at 20 min after injection. A delayed uptake was observed in the stomach (12.8% ± 2.4% ID/g) and urinary bladder (8.7 ± 5.2% ID/g) at 3 and 6 h after injection, respectively. ^123^I-14C5 was cleared mainly by the kidneys, with 40.7 ± 2.9% ID/g being excreted in urine at 48 h after injection, which represents 90.8% of the total excreted radioactivity. Fecal excretion 48 h after tracer injection (4.1 ± 1.0% ID/g) contributed only 9.2% to the total excreted activity.

Burvenich et al. (8) ex vivo performed biodistribution and in vivo imaging studies after injection of ^131^I-14C5 in nude mice bearing an A549 lung carcinoma (high 14C5 antigen expression) or a LoVo colon carcinoma tumor (low 14C5 antigen expression). Tumor radioactivity was measured at 1, 6, 24, and 48 h after tracer injection. The highest tumor uptake was observed with A549 tumors at 24 hours after injection (10.4 ± 0.8% ID/g, n = 5) but was not significantly higher than LoVo tumors (9.3 ± 0.8% ID/g, n = 5) at 24 hours after injection. Both the tumors were visualized at 6 h by planar gamma imaging. The highest tumor/flank ratios were obtained at 48 h after injection with 5.2 ± 1.8 for A549 and 2.0 ± 0.3 for LoVo. Co-injection of 1 μg ^131^I-14C5 with 300 μg unlabeled 14C5 inhibited the accumulation of radioactivity in A549 tumors by 50% at 24 h after injection. No blocking experiment was performed in mice bearing LoVo tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=radioisotopes%2014C5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Coene E., Schelfhout A.M., De Ridder L., De Potter C.R. (1997). Generation of a monoclonal antibody directed against a human cell substrate adhesion molecule and the expression of the antigen in human tissues. Hybridoma.
5 De Potter C.R., Schelfhout A.M., De Smet F.H., Van Damme S., de Ridder L., Dhont E., van Emmelo J. (1994). A monoclonal antibody directed against a human cell membrane antigen prevents cell substrate adhesion and tumor invasion. Am J Pathol.
6 Burvenich I., Schoonooghe S., Vervoort L., Dumolyn C., Coene E., Vanwalleghem L., Van Huysse J., Praet M., Cuvelier C., Mertens N., De Vos F., Slegers G. (2008). Monoclonal antibody 14C5 targets integrin alphavbeta5. Mol Cancer Ther.
7 Lahorte C.M., Bacher K., Burvenich I., Coene E.D., Cuvelier C., De Potter C., Thierens H., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Radiolabeling, biodistribution, and dosimetry of (123)I-mAb 14C5: a new mAb for radioimmunodetection of tumor growth and metastasis in vivo. J Nucl Med.
8 Burvenich I., Schoonooghe S., Cornelissen B., Blanckaert P., Coene E., Cuvelier C., Mertens N., Slegers G. (2005). In vitro and in vivo targeting properties of iodine-123- or iodine-131-labeled monoclonal antibody 14C5 in a non-small cell lung cancer and colon carcinoma model. Clin Cancer Res.